# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-polyethylene glycol 27 anti–tumor-associated glycoprotein 72 diabody

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-polyethylene glycol 27 anti–tumor-associated glycoprotein 72 diabody
Abbreviated name: | ^64^Cu-PEG27 AVP04-07
Synonym: | ^64^Cu-DOTA-PEG27-Cys-VS-AVP04-07
Agent Category: | Antibodies (diabodies)
Target: | Tumor-associated glycoprotein 72 (TAG-72)
Target Category: | Antigens
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=antibody+fragments+and+molecular+imaging)]

Antibody fragments such as diabodies and minibodies are ideal for molecular imaging because of their compact size and efficient antigen binding (1-4). However, most radiometal-labeled antibody fragments exhibit high kidney retention, which leads to decreased absolute tumor uptake (5-7). In the case of radiometals such as ^64^Cu, which have greater tumor retention than radioiodine labels, the advantage is offset by prolonged kidney retention. Use of ^124^I results in reduced kidney uptake due to metabolism and redistribution, but at the expense of lower tumor uptake (1, 8, 9).

An approach to avoid the kidney retention issue is to increase the apparent molecular weight of antibody fragments through attachment of polyethylene glycol (PEG) (5). This approach has been successfully applied to the engineered antibody fragments against carcinoembryonic antigen (CEA), CD3, and others (5, 10). Increased tumor retention, longer serum half-life (t_1/2_), and decreased kidney uptake have been observed for PEGylated fragments compared with non-PEGylated forms (5, 11). Li et al. reported that attachment of 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) and PEG3400 to anti-CEA diabody can significantly reduce kidney uptake of the diabody compared with kidney uptake of the parental diabody while preserving high tumor uptake (5, 12). Li et al. further generated a PEGylated (PEG3400) anti–tumor-associated glycoprotein 72 (TAG-72) diabody (AVP04-07), which reduces kidney retention to levels usually seen with intact immunoglobulin G. Kidney uptake appears to be a function of apparent molecular size (as modified by PEG) and other less defined factors intrinsic to a diabody (1). However, PEG3400 is less than ideal for clinical use because of its inherent polydispersity and the consequent inability to manufacture products that are easy to characterize chemically. Oversubstitution may also inhibit the immunoreactivity of antibody fragments. In the case of anti-CEA diabody, Li et al. showed that it is necessary to limit the number of PEG3400 to approximately one per monomer (5). Li et al. therefore evaluated the effect of monodispersed PEG on the kidney retention and tumor uptake of anti-TAG-72 diabody (1). The investigators synthesized monodispersed PEG (DOTA-PEG27-Cys-VS, where Cys-VS is vinyl sulfone conjugated to the thiol of cysteine) and conjugated this to the amino groups on the anti-TAG-72 diabody (named as PEG27 AVP04-07). Biodistribution studies with ^111^In-labeled PEG27 AVP04-07 demonstrated low kidney uptake without reduction of the tumor uptake and tumor/blood ratio. Positron emission tomography (PET) imaging with ^64^Cu-labeled PEG27 AVP04-07 (^64^Cu-PEG27 AVP04-07) showed high-contrast tumor images (tumor/blood ratio: 8) within 24 h after injection (1).

### Related Resource Links:

- MICAD chapters on TAG-72 antigen (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=anti-TAG-72+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- MICAD chapters on antibody fragments (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=antibody+fragments+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Nucleotide sequences of TAG-72 (http://www.ncbi.nlm.nih.gov/nucleotide/?term=TAG-72)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Li+and+TAG-72+diabody)]

The parental AVP04-07 diabody was generated on the basis of the V-domains from the parent CC49 antibody and the derivative single-chain Fv (scFv) fragments (1, 13). The scFv fragments are orientated as V_H_–V_L_ (where V_H_ and V_L_ are the variable domains of heavy and light chains, respectively) joined by a G_4_S linker and have a C-terminal His_6_ tail. To construct PEG27 AVP04-07, monodispersed DOTA-PEG27-Cys-VS was first synthesized by coupling N-FMOC-amido-PEG27 acid to Cys-polystyrene Wang resin, followed by reaction with a 10-molar excess of VS. Conjugation of the DOTA-PEG27-Cys-VS to the surface lysines of the diabody was carried out at pH 9.0 at a molar ratio of 50:1.

Radiometal labeling was performed using ^111^InCl_3_ or ^64^CuCl_2_ as described in previous reports (1, 12). The radiolabeled materials were purified on Superdex-75 columns. Radiolabeling yields were typically 70–90%. The apparent molecular weight and the degree of PEG27 substitution per monomer diabody were not described in detail for both ^111^In- and ^64^Cu-labeled conjugates (^111^In- and ^64^Cu-PEG27 AVP04-07). The ^111^In- and ^64^Cu-labeled DOTA-Cys-VS-PEG3400-AVP04-07 conjugates (referred to as ^111^In- and ^64^Cu-AVP04-07-PEG3400) were synthesized similarly. The apparent molecular weight of the PEG3400 derivatives was 105 kDa. The radiochemical purity and the specific activity were not reported for either conjugate.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Li+and+TAG-72+diabody)]

Binding of AVP04-07 diabody to the TAG-72 antigen was determined with bovine submaxillary mucin in a column shift assay (Superdex 200) (1). The AVP04-07 diabody showed >99% immunoreactivity. No data were described for the immunoreactivity of the ^111^In- and ^64^Cu-labeled conjugates.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Li+and+TAG-72+diabody)]

A biodistribution study was performed in athymic nude mice bearing LS-174T xenografts (1). In the case of ^111^In-AVP04-07-PEG3400, kidney uptake was 8.4% injected dose per gram tissue (ID/g) at 24 h; uptake was 98% ID/g for the non-PEGylated form. The large reduction of kidney uptake with PEGylation was accompanied by an increase in tumor uptake from 22% ID/g (non-PEGylated) to 46% ID/g (PEGylated) at 24 h. The increased tumor retention is evidently due to the prolonged blood clearance of the PEGylated diabody (t_1/2β_, 36 h) versus the non-PEGylated diabody (t_1/2β_, 18 h). Biodistribution results for ^111^In-PEG27 AVP04-07 were nearly equivalent to those for ^111^In-AVP04-07-PEG3400. At 24 h after injection, kidney uptake of ^111^In-PEG27 AVP04-07 was 8.3% ID/g, tumor uptake was 49% ID/g, and the tumor/blood ratio was 4.2:1.

PET imaging demonstrated modest tumor uptake (19.6% ID/g at 46 h) and high kidney uptake (37.4% ID/g at 46 h) for the ^64^Cu-labeled non-PEGylated AVP04-07 within 2 days after injection. In contrast, ^64^Cu-PEG27 AVP04-07 showed relatively little kidney and liver uptake (6.7% and 8.4% ID/g at 46 h, respectively) over the same period and high tumor uptake (45.1% ID/g at 46 h) as early as 21–22 h. The results were similar to those obtained with the ^111^In-labeled conjugate.

In summary, the PEGylated diabody outperformed the non-PEGylated form in terms of both absolute tumor uptake and tumor/blood ratio for both ^111^In and ^64^Cu labels. The results obtained by Li et al. suggested that even PEGs of modest molecular size are efficient in reducing kidney uptake and that the choice of radiometal labels has little effect on the biodistribution. Monodispersed DOTA-PEGylated diabody conjugates are more suitable for imaging of human TAG-72–positive tumors (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Li L., Turatti F., Crow D., Bading J.R., Anderson A.L., Poku E., Yazaki P.J., Williams L.E., Tamvakis D., Sanders P., Leong D., Raubitschek A., Hudson P.J., Colcher D., Shively J.E. (2010). Monodispersed DOTA-PEG-Conjugated Anti-TAG-72 Diabody Has Low Kidney Uptake and High Tumor-to-Blood Ratios Resulting in Improved 64Cu PET. J Nucl Med.
2 Kortt A.A., Dolezal O., Power B.E., Hudson P.J. (2001). Dimeric and trimeric antibodies: high avidity scFvs for cancer targeting. Biomol Eng.
3 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
4 Wu A.M., Olafsen T. (2008). Antibodies for molecular imaging of cancer. Cancer J.
5 Li L., Yazaki P.J., Anderson A.L., Crow D., Colcher D., Wu A.M., Williams L.E., Wong J.Y., Raubitschek A., Shively J.E. (2006). Improved biodistribution and radioimmunoimaging with poly(ethylene glycol)-DOTA-conjugated anti-CEA diabody. Bioconjug Chem.
6 Li L., Olafsen T., Anderson A.L., Wu A., Raubitschek A.A., Shively J.E. (2002). Reduction of kidney uptake in radiometal labeled peptide linkers conjugated to recombinant antibody fragments. Site-specific conjugation of DOTA-peptides to a Cys-diabody. Bioconjug Chem.
7 Trejtnar F., Laznicek M. (2002). Analysis of renal handling of radiopharmaceuticals. Q J Nucl Med.
8 Schibli R., Schubiger P.A. (2002). Current use and future potential of organometallic radiopharmaceuticals. Eur J Nucl Med Mol Imaging.
9 Lin, X., J. Xie, and X. Chen, Protein-based tumor molecular imaging probes. Amino Acids, 2010
10 Olafsen T., Cheung C.W., Yazaki P.J., Li L., Sundaresan G., Gambhir S.S., Sherman M.A., Williams L.E., Shively J.E., Raubitschek A.A., Wu A.M. (2004). Covalent disulfide-linked anti-CEA diabody allows site-specific conjugation and radiolabeling for tumor targeting applications. Protein Eng Des Sel.
11 Delgado C., Pedley R.B., Herraez A., Boden R., Boden J.A., Keep P.A., Chester K.A., Fisher D., Begent R.H., Francis G.E. (1996). Enhanced tumour specificity of an anti-carcinoembrionic antigen Fab' fragment by poly(ethylene glycol) (PEG) modification. Br J Cancer.
12 Li L., Bading J., Yazaki P.J., Ahuja A.H., Crow D., Colcher D., Williams L.E., Wong J.Y., Raubitschek A., Shively J.E. (2008). A versatile bifunctional chelate for radiolabeling humanized anti-CEA antibody with In-111 and Cu-64 at either thiol or amino groups: PET imaging of CEA-positive tumors with whole antibodies. Bioconjug Chem.
13 Pavlinkova G., Beresford G.W., Booth B.J., Batra S.K., Colcher D. (1999). Pharmacokinetics and biodistribution of engineered single-chain antibody constructs of MAb CC49 in colon carcinoma xenografts. J Nucl Med.